# ^99m^Tc-Ac-Lys(DTPA)-Tyr-Lys(DTPA)-Lys(thiosemicarbazonyl-glyoxyl-cysteinyl-)-NH2 (IMP-192)

Chemical name: | [^99m^Tc]-Labeled Ac-Lys(DTPA)-Tyr-Lys(DTPA)-Lys(thiosemicarbazonyl-glyoxyl-cysteinyl-)-NH_2_ (IMP-192)
Abbreviated name: | [^99m^Tc]-IMP-192
Synonym:
Agent Category: | Compound
Target: | Bispecific PAM4 antibody
Target Category: | Antibody
Method of detection: | Single photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PAM4&cmd=DetailsSearch)]

The majority of individuals suffering from pancreatic adenocarcinoma (PAC) do not survive for more than 1 year after diagnosis and fewer than 1% of these patients live beyond 5 years (1). Although surgical resection of the cancer is a possible intervention for this disease only 10 – 25% of the patients are considered suitable for this treatment because usually by the time that neoplasm is detected the malignancy has metastasized to other organs and the tumor load in the patient is too high to warrant surgery (2). Patients with nonresectable PAC are treated either with gemcitabine (http://www.cancer.gov/cancertopics/druginfo/gemcitabinehydrochloride) or radiotherapy or a combination of the two, however, these treatments are not curative because they only prolong survival and improve the quality of life of the patient (2). The detection of this cancer at an early stage can facilitate proper staging of the disease so that a suitable treatment regimen can be initiated to possibly improve patient prognosis (3). In this regard the monoclonal antibody (mAb), PAM4, which specifically targets mucin 1 (MUC1), a glycoprotein, that is overexpressed only in PAC tumors was developed, radiolabeled with ^131^I or ^111^In and shown to detect neoplastic tumors with scintigraphy in patients having pancreatic malignancies (4). However, intact radiolabeled antibodies are of limited utility to visualize cancerous lesions due to their large size (~150 kDa) and long circulating half-life (5). To amplify the signal obtained from an imaging agent that can be used to detect malignant tumors noninvasively, investigators have developed and evaluated a variety of strategies in preclinical studies in animals such as pretargeting the cancer lesion with a suitable mAb (or its derivative) followed by exposing the animals to an appropriate radiolabeled small molecular weight ligand that targets the mAb or its derivative. This technique has been shown to generate a higher signal-to-noise ratios during imaging compared to ratios obtained with a directly labeled mAb alone (6-8). Use of the pretargeting technique for the imaging and therapy of cancer has been discussed elsewhere (9, 10).

Cardillo et al. developed a bispecific F(ab’)_2_ mAb (bsPAM4; bsmAb) by cross-linking a PAM4 Fab’ fragment (binds the MUC-1 antigen) to a murine anti-indium-diethylenetriaminepentaacetic acid (DTPA) mAb Fab’ fragment (binds the peptide heptan antigen) and used the unlabeled bsmAb to pretarget human CaPan-1 cell xenograft PAC tumors in nude mice (4). After the bsmAb was cleared from blood circulation the animals were injected with a radiolabeled peptide heptan to visualize the PAC lesions with whole body scintigraphy. To confirm the tumor targeting specificity and delivery of bsPAM4 to the tumor (the pretargeting bsmAb) the biodistribution of this bsmAb was investigated in mice bearing human PAC tumors using ^125^I-labeled bsPAM4 ([^125^I]-bsPAM4) (4). Subsequently two groups of animals pretargeted with bsPAM4 were separately injected with radiolabeled peptide haptens, ^111^In-labeled Ac-Phe-Lys(DTPA)-Tyr-Lys(DTPA)-NH_2_ ([^111^In]-IMP-156) and ^99^Tc-labeled Ac-Lys(DTPA)-Tyr-Lys(DTPA)-Lys(thiosemicarbazonyl-glyoxyl-cysteinyl-)-NH_2_ ([^99m^Tc]-IMP-192), that specifically bind the anti-indium-DTAP mAb Fab’ arm of the bsmAb and the biodistribution of these radiolabeled peptides was investigated in the tumor bearing rodents. This chapter describes the biodistribution characteristics of [^99m^Tc]-IMP-192. The biodistribution of radioiodinated bsPAM4 in non-pretargeted mice (11) and the biodistribution and imaging studies performed with [^111^In]-IMP-156 in mice pretargeted with bsPAM4 (12) are discussed in separate chapters of MICAD (www.micad.nih.gov).

### Other Sources of Information

Peptide haptens [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=peptide%20haptens&cmd=DetailsSearch)]

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bispecific+antibody) with bispecific antibodies

Application of multivalent antibodies [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=application%20of%20multivalent%20antibodies&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-bsPAM4%20synthesis&cmd=DetailsSearch)]

The synthesis of bsPAM4 and another bsmAb, bispecific retuximab (bsRIT; for use as a control) has been described by Cardillo et al. (4). The cross-linked bsmAbs were purified by size-exclusion chromatography (SEC) and the ratio of each Fab’ fragment in the complex was determined to be 1:1 with high performance liquid chromatography. The two bsmAbs were labeled with ^125^I using the chloramine-T method to obtain [^125^I]-bsPAM4 and [^125^I]-bsRIT as described elsewhere (4). [^125^I]-bsPAM4 and [^125^I]-bsRIT were reported to have a specific activity (SA) of 492.2 MBq/mg (11.6 mCi/mg) and 403.3 MBq/mg (10.9 mCi/mg), respectively. The radiochemical purity and yield of both the radioiodinated bsmAbs was not reported.

IMP-192 was obtained from a commercial source and labeled with ^99m^Tc as described elsewhere (4). The number of Tc atoms bound to each molecule of IMP-192 (that has two DTPA sites within the structure as described above) was not reported. The SA of [^99m^Tc]-IMP-192 was reported to be 77.7 MBq/nmol (2.1 mCi/nmol) and the radiolabeled peptide was reported to contain no aggregates and <2% unbound radioactivity as determined by instant thin layer chromatography. In an earlier study the radiochemical yield of the ^99m^Tc-labeled peptide was reported to be 94-99% and had a SA of up to 67.7 GBq/mmol (1.83 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=IMP-192%20in%20vitro&cmd=DetailsSearch)]

Karacay et al. reported that IMP-192 can be stored in a freeze dried form at -20^o^ C for prolonged periods (13). The in vitro stability of [^99m^Tc]-IMP-192 in normal saline (0.9% sodium chloride), 1% human serum albumin and 10 mM cysteine was 96%, 96% and 89%, respectively, as determined by reversed-phase high performance liquid chromatography (13).

To investigate the bsmAb binding characteristics of [^99m^Tc]-IMP-192, 0.15 pmol of the labeled peptide was mixed with 10 pmol bsPAM4 in presence of excess MUC1 (200 μg) and the mixture was incubated at 37^o^ C for 1 h (4). Subsequently size-exclusion chromatography of the mixture revealed that 81% of the tracer bound to bsPAM4 and of the total bsmAb bound fraction 85% of the label was in the MUC1 fraction, 11% in the non-MUC1-reactive bsPAM4 fraction and 4% of the radiocompound bound nonspecifically to the MUC1 antigen.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-bsPAM4%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]-IMP-192 was investigated in athymic nu/nu mice bearing human PAC CaPan-1 cell tumors (n = 14 mice/group) that were pretargeted with either [^125^I]-bsPAM4 or [^125^I]-bsRIT (control bsmAb) (4). A group of animals was injected with 10 μCi (150 pmol) [^125^I]-bsPAM4 and another other group received 10 μCi (150 pmol) of [^125^I]-bsRIT. Two other groups of animals received the labeled peptides alone. After 40 h the mice were injected with 28 μCi (15 pmol) [^99m^Tc]-IMP-192 and the animals were euthanized at 3 and 24 h post injection (p.i.; i. e. 43 and 64 h after administration of the bsmAbs). All organs of interest, including the tumors, were removed from the mice and the amount of radioactivity in the various tissues was determined. Data obtained from this study was presented as percent of injected dose per gram tissue (%ID/g).

At 3 h after injecting the radiolabeled peptide the amount of radioactivity in the tumor from animals pretreated with bsPAM4 was reported to be 16.8 ± 4.8%ID/g (P < 0.0005) compared to 1.1 ± 0.2%ID/g in tumors of the bsRIT pretreated animals (4). Similarly, at 24 h after the treatment with [^99m^Tc]-IMP-192 mice pretreated with bsPAM4 had an accumulation of 12.9 ± 4.2%ID/g (P < 0.0008) compared to 0.4 ± 0.03%ID/g in animals pretreated with bsRIT. Animals injected with the labeled peptide alone showed negligible uptake of radioactivity at both the time points (0.2 ± 0.05%ID/g, P < 0.0004, and 0.06 ± 0.02%ID/g, P < 0.0002 at 3 h and 24 h after treatment, respectively). At 24 h after treatment the tumor-to-nontumor ratios with [^99m^Tc]-IMP-192 for all tissues were higher than the ratios obtained from animals treated with [^125^I]-bsPAM4 alone. In animals pretreated with bsPAM4 the tumor-to-blood ratio with the ^99m^Tc-labeled peptide was 80:1 compared to a ratio of 4:1 obtained with the non-pretargeted mice injected with [^125^I]-bsPAM4 alone (P<0.0002).

From these studies the investigators concluded that [^99m^Tc]-IMP-192was suitable to target PAC xenograft tumors in rodents pretargeted with bsPAM4 in rodents (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B125I%5D-PAM4%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B125I%5D-PAM4%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B125I%5D-PAM4%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies described in this chapter were supported by National Institutes of Health grants CA-54425 and CA92723.

## References

1 Gold D.V., Goldenberg D.M., Karacay H., Rossi E.A., Chang C.H., Cardillo T.M., McBride W.J., Sharkey R.M. (2008). A novel bispecific, trivalent antibody construct for targeting pancreatic carcinoma. Cancer Res.
2 Gold D.V., Cardillo T., Goldenberg D.M., Sharkey R.M. (2001). Localization of pancreatic cancer with radiolabeled monoclonal antibody PAM4. Crit Rev Oncol Hematol.
3 Gold D.V., Goggins M., Modrak D.E., Newsome G., Liu M., Shi C., Hruban R.H., Goldenberg D.M. (2010). Detection of early-stage pancreatic adenocarcinoma. Cancer Epidemiol Biomarkers Prev.
4 Cardillo T.M., Karacay H., Goldenberg D.M., Yeldell D., Chang C.H., Modrak D.E., Sharkey R.M., Gold D.V. (2004). Improved targeting of pancreatic cancer: experimental studies of a new bispecific antibody, pretargeting enhancement system for immunoscintigraphy. Clin Cancer Res.
5 Ahlgren S., Orlova A., Wallberg H., Hansson M., Sandstrom M., Lewsley R., Wennborg A., Abrahmsen L., Tolmachev V., Feldwisch J. (2010). Targeting of HER2-expressing tumors using 111In-ABY-025, a second-generation affibody molecule with a fundamentally reengineered scaffold. J Nucl Med.
6 Forster G.J., Santos E.B., Smith-Jones P.M., Zanzonico P., Larson S.M. (2006). Pretargeted radioimmunotherapy with a single-chain antibody/streptavidin construct and radiolabeled DOTA-biotin: strategies for reduction of the renal dose. J Nucl Med.
7 Liu G., Dou S., Pretorius P.H., Liu X., Chen L., Rusckowski M., Hnatowich D.J. (2010). Tumor pretargeting in mice using MORF conjugated CC49 antibody and radiolabeled complimentary cMORF effector. Q J Nucl Med Mol Imaging.
8 Uppal J.K., Varshney R., Hazari P.P., Chuttani K., Kaushik N.K., Mishra A.K. (2011). Biological evaluation of avidin-based tumor pretargeting with DOTA-Triazole-Biotin constructed via versatile Cu(I) catalyzed click chemistry. J Drug Target.
9 Goldenberg D.M., Sharkey R.M. (2010). Radioactive antibodies: a historical review of selective targeting and treatment of cancer. Hosp Pract (Minneap).
10 Sharkey R.M., Goldenberg D.M. (2011). Cancer radioimmunotherapy. Immunotherapy.
11 Chopra, A., 125I-Labeled anti-mucin 1 bispecific antibody bsPAM4. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., 111In-labeled Ac-Phe-Lys(DTPA)-Tyr-Lys(DTPA)-NH2 (IMP-156). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Karacay H., McBride W.J., Griffiths G.L., Sharkey R.M., Barbet J., Hansen H.J., Goldenberg D.M. (2000). Experimental pretargeting studies of cancer with a humanized anti-CEA x murine anti-[In-DTPA] bispecific antibody construct and a (99m)Tc-/(188)Re-labeled peptide. Bioconjug Chem.